# [O-methyl-^11^C]2-{4-[4-(7-Methoxynaphthalen-1-yl)piperazin-1-yl]butyl}-4-methyl-2H-[1,2,4]triazine-3,5-dione

Chemical name: | [O-methyl-^11^C]2-{4-[4-(7-Methoxynaphthalen-1-yl)piperazin-1-yl]butyl}-4-methyl-2H-[1,2,4]triazine-3,5-dione
Abbreviated name: | [^11^C]MPT
Synonym: | [^11^C]F1146
Agent Category: | Compound
Target: | 5-HT_1A_ serotonin receptors
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29)]

[O-methyl-^11^C]2-{4-[4-(7-Methoxynaphthalen-1-yl)piperazin-1-yl]butyl}-4-methyl-2H-[1,2,4]triazine-3,5-dione ([^11^C]MPT) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-hydroxytryptamine 1A (5-HT_1A_)) receptors in the central nervous system (1). It is a selective 5-HT_1A_ agonist labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1, 2).

The 5-HT neurotransmission system comprises mainly neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord (3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which also contain several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family, with the 5-HT_1A_ subtype located primarily in the limbic forebrain (the hippocampus, entorhinal cortex ,septum, and raphe) (4, 5). 5-HT_1A_ receptors appear to function both as presynaptic (somatodendritic) autoreceptors in the raphe nuclei and as postsynaptic receptors in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and it is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders (6). A radioligand that can be used to assess the in vivo densities of 5-HT_1A_ receptors and their changes may facilitate investigation of the relationship of these receptors to various neuropsychiatric diseases and aid in the design of novel drugs for their treatment.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors (2). Various compounds have been radiolabeled for visualization and quantification of these receptors (7). 5-HT_1A_ receptors appear to exist in the high (HA) and low (LA) agonist affinity states. Antagonist ligands bind to both the HA and LA conformations, whereas agonist ligands bind to the HA state, which is coupled to G-protein. WAY 100635 was developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5-HT_1A_ receptors at both pre- and postsynaptic sites. WAY 100635 radiolabeled with ^11^C at the carbonyl position is an effective radioligand but it is rapidly cleared and metabolized. Analogs of WAY 100635 that bear bulkier cycloalkylcarbonyl groups appear to be more resistant to amide hydrolysis. However, the added lipophilicity also reduces receptor affinity (8). Although 5-HT_1A_ receptor agonist ligands can elicit pharmacologic effects, there are some distinct potential applications of radiolabeled 5-HT_1A_ receptor agonist ligands because they behave like serotonin, which binds preferentially to the HA sites (1, 9). Kumar et al. (1) selected MPT for development as a radiolabeled 5-HT_1A_ receptor agonist probe because of its high affinity (pK_i_ = 10.49) and favorable calculated lipophilicity (clogP = 1.8) (10, 11)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20synthesis)]

Kumar et al. (1) designed the synthesis of MPT in five steps from the starting material of commercially available 6-azauracil. Briefly, 6-azauracil was selectively acetylated at the 2-position by refluxing in acetic anhydride. The resulting product was methylated at the 4-position by sodium hydride in N,N-dimethylformamide (DMF) and methyl iodide followed by treatment with catalytic p-TsOH in refluxing ethanol. This methylated compound was alkylated with 1-bromo-4-chlorobutane in DMF and sodium hydride to produce 2-(4-chlorobutyl)-4-methyl-2H-[1,2,4]triazine-3,5-dione. This compound was used to prepare the precursors for MPT and [^11^C]MPT. To prepare the radiolabeling precursor, 8-aminonaphthalen-2-ol and bis-(2-chloroethyl)amine in poly(ethylene glycol) were reacted in microwave conditions to yield 8-piperazin-1-ylnaphthalen-2-ol. This was coupled with 2-(4-chlorobutyl)-4-methyl-2H-[1,2,4]triazine-3,5-dione to yield the desmethyl precursor 2-{4-[4-(7-hydroxynaphthalen-1-yl)piperazin-1-yl]butyl}-4-methyl-2H-[1,2,4]triazine-3,5-dione, which was used for radiolabeling. This precursor was treated with [^11^C]CH_3_OTf in acetone in the presence of 10 μl of 5 M sodium hydroxide at room temperature. The radiolabeled MPT was purified by high-performance liquid chromatography (HPLC) and passed through a C-18 Sep-Pak cartridge. The radiochemical yield at the end of synthesis was 25 ± 5% (n = 15), and the chemical and radiochemical purities were >99%. The specific activity of [^11^C]MPT was 55.5 ± 11.1 TBq/mmol (1,500 ± 300 Ci/mmol; n = 10) at the end of bombardment (EOB). The average time of labeling was 30 min from the time of EOB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20in%20vitro)]

The partition coefficient (logP_OCT_) of [^11^C]MPT was determined to be 2.2 by the standard shake-flask method by mixing the radioligand in 1-octanol and phosphate-buffered saline (pH 7.4) (1). The inhibitory constant value (K_i_) of unlabeled MPT for 5-HT_1A_ was found to be 1.36 ± 0.16 nM by use of the competition binding studies with [^3^H]8-OH-DPAT (5-HT_1A_ receptor agonist) in membrane fractions from Chinese hamster ovary (CHO) cells that had a density of 8 pmol/mg 5-HT_1A_ receptors. The K_i_ of MPT for other 5-HT receptor subtypes (5-HT_2A_ to 5-HT_7_) ranged from 9.1 (5-HT_7_) to >10,000 nM (5-HT_3_). In comparison, serotonin had a K_i_ value of 1.58 nM for the 5-HT_1A_ receptors. An in vitro agonist-stimulated [^35^S]GTPγS binding assay indicated that MPT was a 5-HT_1A_ receptor agonist with an affinity greater than that of endogenous serotonin. The EC_50_ values of MPT and serotonin were determined to be 0.05 nM and 0.5 nM, respectively. In the inhibition assay of forskolin-stimulated cAMP accumulation, the EC_50_ values of MPT and serotonin were 0.01 nM and 1 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20%28primate%20NOT%20human%29)]

Kumar et al. (1) evaluated the in vivo properties of [^11^C]MPT in baboons. For each study, a single male baboon received an i.v. dose of 185 ± 18.5 MBq (5 ± 0.5 mCi) for PET imaging studies. The PET imaging showed that [^11^C]MPT rapidly penetrated the blood–brain barrier and accumulated in brain regions known to have high densities of 5-HT_1A_ receptors. The cerebellum had the lowest radioactivity level of [^11^C]MPT. There was a high correlation between the volume of distribution (V_T_) of [^11^C]WAY 100635 and the V_T_ of [^11^C]MPT. When 0.5 mg/kg unlabeled WAY 100635 or 2 mg/kg 8-OH-DPAT was given 20 min before [^11^C]MPT administration, the radioactivity levels in all brain regions were reduced to the same level as the cerebellar reference region. Blocking studies with a 5-HT_2A_ antagonist and a dopamine antagonist showed that [^11^C]MPT did not have significant affinity for 5-HT_2A_ or dopamine receptors.

HPLC analysis of [^11^C]MPT metabolite in baboons indicated that [^11^C]MPT underwent fast metabolism, and the percentages (n = 15) of unchanged [^11^C]MPT in the total plasma radioactivity were 90 ± 2% (2 min), 87 ± 3% (4 min), 65 ± 5% (12 min), 30 ± 5% (30 min), 20 ± 3% (60 min), and 12 ± 3% (90 min) (1). Only polar metabolites were discovered in the plasma samples.

## Human Studies

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28A%20novel%205-HT1A%20receptor%20agonist%20positron%20emission%20tomography%20ligand%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH P50 MH62185.

## References

1 Kumar J.S., Majo V.J., Hsiung S.C., Millak M.S., Liu K.P., Tamir H., Prabhakaran J., Simpson N.R., Van Heertum R.L., Mann J.J., Parsey R.V. (2006). Synthesis and in vivo validation of [O-methyl-11C]2-{4-[4-(7-methoxynaphthalen-1-yl)piperazin- 1-yl]butyl}-4-methyl-2H-[1,2,4]triazine-3,5-dione: a novel 5-HT1A receptor agonist positron emission tomography ligand. J Med Chem.
2 Bantick R.A., Rabiner E.A., Hirani E., de Vries M.H., Hume S.P., Grasby P.M. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
3. Sunderland, P.M., Structure and function of the nervous system, in Pathophysiology: The biologic basis for disease in adults and children, K.L. McCance, and S.H. Huether, Editor. 1994, Mosby-Year Book, Inc.: St. Louis, MO. p. 397-436.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Passchier J., van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
6 Lang L., Jagoda E., Schmall B., Vuong B.K., Adams H.R., Nelson D.L., Carson R.E., Eckelman W.C. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
7 Tauscher J., Verhoeff N.P., Christensen B.K., Hussey D., Meyer J.H., Kecojevic A., Javanmard M., Kasper S., Kapur S. (2001). Serotonin 5-HT1A receptor binding potential declines with age as measured by [11C]WAY-100635 and PET. Neuropsychopharmacology.
8 Houle S., DaSilva J.N., Wilson A.A. (2000). Imaging the 5-HT(1A) receptors with PET: WAY-100635 and analogues. Nucl Med Biol.
9 Watson J., Collin L., Ho M., Riley G., Scott C., Selkirk J.V., Price G.W. (2000). 5-HT(1A) receptor agonist-antagonist binding affinity difference as a measure of intrinsic activity in recombinant and native tissue systems. Br J Pharmacol.
10 Koek W., Vacher B., Cosi C., Assie M.B., Patoiseau J.F., Pauwels P.J., Colpaert F.C. (2001). 5-HT1A receptor activation and antidepressant-like effects: F 13714 has high efficacy and marked antidepressant potential. Eur J Pharmacol.
11 Bruins Slot L.A., Koek W., Tarayre J.P., Colpaert F.C. (2003). Tolerance and inverse tolerance to the hyperalgesic and analgesic actions, respectively, of the novel analgesic, F 13640. Eur J Pharmacol.